# [Carbonyl-^11^C]N-(2-(1-(4-(2-Methoxyphenyl)-piperazinyl)ethyl)-N-pyridinyl)cyclohexanecarboxamide

Chemical name: | [Carbonyl-^11^C]N-(2-(1-(4-(2-Methoxyphenyl)-piperazinyl)ethyl)-N-pyridinyl) cyclohexanecarboxamide
Abbreviated name: | [Carbonyl-^11^C]WAY 100635
Synonym: | ^11^C-WAY, ^11^C-WAY 100635
Agent Category: | Compound
Target: | 5-HT_1A_ receptors
Target Category: | Receptor-ligand binding
Method of detection: | Positron Emission Tomography (PET)
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%5B11C%5DWAY-100635)]

[Carbonyl-^11^C]N-(2-(1-(4-(2-Methoxyphenyl)-piperazinyl)ethyl)-N-pyridinyl) cyclohexanecarboxamide ([carbonyl-^11^C]WAY 100635) is a radioligand developed for positron emission tomography (PET) imaging of serotonin-1A (5-HT_1A_) receptors in the central nervous system (1). It is a selective 5-HT_1A_ antagonist radiotracer labeled with ^11^C, a positron emitter with a physical t_½_ of 20.4 min (2).

The serotonin (5-hydroxytryptamine 5-HT) neurotransmission system consists mainly of neurons in the brainstem, with nerve tracts extending from these neurons to many areas of the brain and spinal cord (3). During firing, the neurons release 5-HT, a neurotransmitter that is involved in the modulation of various important physiological functions and behavior, such as thermoregulation, cardiovascular function, aggressive and sexual behavior, mood, appetite, and the sleep–wake cycle (1). The effects of 5-HT are mediated by as many as seven classes of receptor populations (5-HT_1_ to 5-HT_7_), and many of which also contain several subtypes (4). There are five receptor subtypes within the G protein-coupled 5-HT_1_ receptor family, and the 5-HT_1A_ subtype is primarily located in the limbic forebrain (the hippocampus, entorhinal cortex and septum) (1, 4). It appears to function both as presynaptic (somatodendritic) autoreceptors in the raphe nuclei and as postsynaptic receptors in the terminal fields. This receptor subtype is involved in the modulation of emotion and the function of the hypothalamus, and is implicated in the pathogenesis of anxiety, depression, hallucinogenic behavior, motion sickness, dementia, schizophrenia, and eating disorders (5). A radioligand that can be used to assess the in vivo densities of 5-HT_1A_ receptors and their changes may facilitate investigation of the relationship of these receptors to various neuropsychiatric diseases and aid in the design of novel drugs for their treatment.

Many psychiatric drugs modulate serotonergic transmission or specifically target the 5-HT_1A_ receptors (2). Many compounds have been radiolabeled and studied for visualization and quantification of these receptors using PET or single-photon emission computed tomography (SPECT). Selective agonists such as 8-hydroxy-N-N-dipropylaminotetralin (8-OH-DPAT) were initially studied, but because they bind to the relatively few 5-HT_1A_ receptors in the high-affinity state, the higher affinity required in that situation was difficult to achieve (6). WAY 100635 has been developed as a highly selective, silent antagonist (possessing no intrinsic agonist activity) of 5HT_1A_ receptors at both presynaptic and postsynaptic sites (7). The initial radiolabel was placed in the O-methoxy position, but studies have shown that this [O-methyl-^11^C] radioligand is metabolized by in vivo amide hydrolysis in primates to a lipophilic radiolabeled amine metabolite that can cross the blood-brain barrier with high affinities for both α_1_-adrenoceptors and 5-HT_1A_ receptors (8, 9). The labeling of WAY 100635 with ^11^C in its carbonyl position provides the current [carbonyl-^11^C]WAY 100635 radioligand which avoids the formation of the undesirable radiolabeled metabolite (8, 10).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%5B11C%5DWAY100635%20AND%20synthesis)]

There were three reported procedures for preparing [carbonyl-^11^C]WAY 100635. Pike and colleagues (11, 12) first reported a simple one-pot procedure. WAY 100635 was synthesized by reacting 2-[1-[4-(2-methoxyphenyl)piperazinyl]]-N-(2-pyridyl)-acetamide with lithium aluminum hydride. The purified ligand (23% yield) was then reacted with ^11^CO_2_ produced by a cyclotron using an O_2_/N_2_ gas target. This procedure had a relatively low radiochemical yield of 0.7%. The procedure was improved and adopted to a remotely controlled production by using immobilized cyclohexylmagnesium chloride as a Grignard reagent in a long polypropylene ubing to trap ^11^CO_2_ and to obtain the desired [carbonyl-^11^C]cyclohexanecarbonyl chloride (by passing thionyl chloride through the tubing) (13). The synthesis time was 45 min, and the radiochemical yield was improved to 3-4% with a >99% radiochemical purity and a specific activity of 192 GBq/µmol (5.24 Ci/µmol) at the end of synthesis (EOS). Hwang et al. (14) reported another improved, one-pot procedure that removed of excess reagents before the final coupling step. They reported a synthesis time of 45 min, a radiochemical yield of 2.5% (1110 ± 481 MBq from 48.1 GBq; 30 ± 13 mCi from 1.3 Ci ^11^CO_2_), and a specific activity of 133 ± 70 GBq/µmol (3.6 ± 1.9 Ci/µmol; n = 40) at the EOS.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5B11C%5DWAY100635%20or%20C-11-WAY100635%29%20AND%20in%20vitro)]

Forster and colleagues (15) reported that the affinity pIC_50_ value of WAY 100635 at 5-HT_1A_ sites to rat hippocampal membranes was 8.87 ± 0.14. This represented a >100-fold selectivity relative to binding at other 5-HT receptors. The in vitro localization of [carbonyl-^11^C]WAY 100635 was studied in postmortem human brain cryosections by incubating the tissue sections with the radioligand for 20 min at room temperature and then processing for whole hemisphere autoradiography (10). The distribution of [carbonyl-^11^C]WAY 100635 was similar to that of ^3^H-labeled WAY 100635 ([O-methyl-^3^H] labeled, K_d_ = 2.5 nM) with high binding in the hippocampus and neocortex. This binding was blocked by 5-HT_1A_ receptor ligands that included buspirone (a parial 5-HT_1A_ receptor agonist), 5-HT, pindolol (a 5-HT_1A_ receptor antagonist) and 8-OH-DPAT.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28C-11-WAY100635%20or%20%5B11C%5DWAY100635%29%20AND%20rodentia)]

Maeda and colleagues (16) in 2001 used PET imaging and ex vivo autoradiography to measure the effect of endogenous serotonin on the in vivo binding properties of [carbonyl-^11^C]WAY 100635 (specific activity = 148-370 GBq/µmol; 4-10 Ci/µmol at the EOS) in rats. In one experiment, 5-HT neurons were destroyed by using 5,7-DHT. In another experiment, the in vivo release of 5-HT was modified by either fenfluramine (10 mg/kg dose; increased 5-HT release) or reserpine (5 mg/kg dose; depletion of 5-HT) treatment. In all of these experiments, no significant change in [carbonyl-^11^C]WAY 100635 (11.1-25.9 MBq/rat; 0.3-0.7 mCi/rat) binding was found in the hippocampus and entorhinal cortex, whereas there was a 40-65% decrease in the raphe nucleus after neuron destruction with 5,7-DHT. It was suggested that this radioligand mainly bound to the postsynaptic 5-HT_1A_ receptors, and the binding was not sensitive to the level of endogenous 5-HT. Hume et al. (17) also used similar techniques to study the in vivo specific binding of [carbonyl-^11^C]WAY 100635 (10.4 MBq/rat; 0.28 mCi/rat) in rats. Administration of fenfluramine (10 mg/kg) resulted in a slight overall reduction (10-20%; significant at P = 0.01) in the hippocampus binding. They also concluded that only a large change in endogenous agonist concentration would affect [carbonyl-^11^C]WAY 100635 binding.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28C-11%20WAY%20100635%20or%20%5B11C%5DWAY%20100635%20or%20%5Bcarbonyl-11C%5DWAY%20100635%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28C-11%20WAY%20100635%20or%20%5B11C%5DWAY%20100635%20or%20%5Bcarbonyl-11C%5DWAY%20100635%5D%20AND%20%28primate%20NOT%20human%29)]

PET imaging studies were performed in cynomolgus monkeys (n = 4) with i.v. administration of 37 MBq (1 mCi) of [carbonyl-^11^C]WAY 100635 (specific activity, 20-60 GBq/µmol; 0.54-1.62 Ci/µmol at the time of i.v. administration; TOA) (18). The mean ratios of radioactivity for the neocortex and raphe nuclei to the cerebellum were 7.8 and 2.7, respectively. The in vivo competitive binding experiment (homologous) and its subsequent Scatchard plot indicated a 5-HT_1A_ receptor density value of 16.2 pmol/ml for the neocortex and 4.5 pmol/ml for the raphe nuclei. Bindings in these areas were reduced or inhibited by pretreatment with unlabeled WAY 100635, 8-OH-DAT (8 mg/kg), buspirone (5 mg/kg) or pindolol (1 mg/kg).

Osman and colleagues (19) performed PET imaging for 90 min in 6 cynomolgus monkeys that received injections of 37 MBq (1 mCi) of [carbonyl- ^11^C]WAY 100635 (specific activity, 80 GBq/µmol; 2.16 Ci/µmol at TOA). The maximum radioactivity in the whole brain was about 5% of the injected dose at 2.5 min after injection. Very high radioactivity was observed in the occipital and temporal cortex, and very low radioactivity was found in the thalamus and cerebellum. The ratios of radioactivity in the occipital cortex to the cerebellum varied from 10 to 16. In comparison with published data from the [O-methyl-^11^C] labeled analog, the distribution of the latter appeared to be consistent with low penetration and retention of polar radioactive metabolities from [carbonyl-^11^C]WAY 100635. High performance liquid chromatography (HPLC) analyses of plasma samples indicated that carbonyl-labeled ^11^C-WAY 100635 was rapidly metabolized. Polar metabolites were detected, and the parent radioligand represented about 19% of the radioactivity in the plasma at 47 min. One of the major metabolites was confirmed to be ^11^C-cyclohexanecarboxylic acid, and other metabolites were found to be more polar.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28C-11-WAY100635%20or%20%5B11C%5DWAY100635%29%20AND%20human)]

Pike et al. (20) in 1995 reported the first PET imaging of healthy volunteers (n = 5), for 20-90 min after injection with [carbonyl-^11^C]WAY 100635 (222 MBq/10 µg; 6 mCi/10 µg at the TOA). High radioactivity was observed in the entorhinal cortex, frontal cortrex, hypothalamus and insula, and the lowest radioactivity was found in the cerebellum. The ratios of radioactivity at 20 min after injection for the medial temporal cortex, insula and cingulate to the cerebellum were 3.1, 2.7 and 2.0, respectively. In another similar study, they described a kinetic analysis of a 270 MBq (7.29 mCi) dose of [carbonyl-^11^C]WAY 100635 (specific activity, 75 GBq/µmol; 2.03 Ci/µmol at TOA) to two healthy subjects (21). With the use of a reference tissue compartmental model, the binding potential (BP) of the medial temporal cortex was shown to be 7.8 for both subjects. The analysis of serum showed that the radioligand was rapidly metabolized to very polar radioactive metabolites that could not enter the brain. This observation was confirmed by Osman and colleagues (19) in their studies of 7 healthy volunteers who received injections of 165-416 MBq/4-10 µg (4.5-11.2 mCi/4-10 µg at theTOA) of [carbonyl-^11^C]WAY 100635, and then PET imaging was used up to 90 min. Radioactivity was mostly observed to be taken up and retained by 5-HT_1A_ receptor-rich regions of the brain. ^11^C-Cyclohexanecarboxylic acid was identified by plasma sample analysis using HPLC as a significant radioactive metabolite of the radioligand.

A PET imaging study of tracer kinetic modeling of [carbonyl-^11^C]WAY 100635 in 6 healthy volunteers described a reference tissue model (the cerebellum as the reference tissue) that was relatively simple to use for the radioligand quantification (22). The BP values derived from this model for the medial temporal cortex, insula cortex, cingulated cortex and raphe nucleus were 7.43-7.65, 6.38-6.61, 4.80-4.85, and 3.91-4.52, respectively. Parsey and colleagues (23) confirmed the usefulness of this model with another study in 5 healthy volunteers.

In a 2005 biodistribution and radiation dosimetry study, 6 healthy volunteers received 243 ± 43 MBq (6.57 ± 1.16 mCi) of [carbonyl-^11^C]WAY 100635 (specific activity, 140 ± 35 MBq/nmol; 3.78 ± 0.95 mCi/nmol at TOA) (24). The data showed that the radioligand was mainly eliminated by the kidneys, and the urinary bladder without catheterization was the critical organ that received the highest mean radiation absorbed dose (0.194 ± 0.0357 mGy/MBq; 718.5 ± 132.2 mrad/mCi). The brain and the kidneys received 0.00369 ± 0.00128 mGy/MBq (13.7 ± 4.7 mrad/mCi) and 0.0348 ± 0.00636 mGy/MBq (128 ± 23.6 mrad/mCi), respectively. The human radiation dose in the kidneys was 6.0 times higher and in the urinary bladder wall was 60.6 times higher than the estimates from rats.

Sargent et al. (25) performed [carbonyl-^11^C]WAY 100635 PET scans in 25 patients with major depressive disorders. They found that their BP values were significantly reduced across many of the regions examined (the frontal, temporal, and limbic cortexes) in both unmedicated (n = 15) and medicated (with selective serotonin reuptake inhibitors) depressed patients when compared with healthy volunteers (n = 18). No difference was found between the unmedicated and medicated patients that indicated that the reduced [carbonyl-^11^C]WAY 100635 binding was not changed by selective serotonin reuptake inhibitor treatment. Other studies also found significant reduction of [carbonyl-^11^C]WAY 100635 binding in patients with recovered depression, late life depression, medial temporal lobe epilepsy, amyotrophic lateral sclerosis, chronic fatigue syndrome, recovered anorexia nervosa, and Parkinson’s disease (26-31).

## References

1 Passchier J, van Waarde A. (2001). Visualisation of serotonin-1A (5-HT1A) receptors in the central nervous system. Eur J Nucl Med.
2 Bantick RA, Rabiner EA, Hirani E, de Vries MH, Hume SP, Grasby PM. (2004). Occupancy of agonist drugs at the 5-HT1A receptor. Neuropsychopharmacology.
4. Lanfumey L, Hamon M 5-HT1 receptors Curr Drug Targets CNS Neurol Disord 2004;3(1):1–10.
5 Lang L, Jagoda E, Schmall B, Vuong BK, Adams HR, Nelson DLRE, Eckelman WC. (1999). Development of fluorine-18-labeled 5-HT1A antagonists. J Med Chem.
6. Tauscher J, Verhoeff NP, Christensen BK, Hussey D, Meyer JH, Kecojevic A, Javanmard M, Kasper S, Kapur S Serotonin 5-HT1A receptor binding potential declines with age as measured by [11C]WAY-100635 and PET Neuropsychopharmacology 2001;24(5):522–530.
7 Cliffe IA. (2000). A retrospect on the discovery of WAY-100635 and the prospect for improved 5-HT(1A) receptor PET radioligands. Nucl Med Biol.
8 Pike VW, Halldin C, Wikstrom H, Marchais S, McCarron JA, Sandell J, Nowicki B, Swahn CG, Osman S, Hume SP, Constantinou M, Andree B, Farde L. (2000). Radioligands for the study of brain 5-HT(1A) receptors in vivo--development of some new analogues of way. Nucl Med Biol.
9 Osman S, Lundkvist C, Pike VW, Halldin C, McCarron JA, Swahn CG, Ginovart N, Luthra SK, Bench CJ, Grasby PM, Wikstrom H, Barf T, Cliffe IA, Fletcher A, Farde L. (1996). Characterization of the radioactive metabolites of the 5-HT1A receptor radioligand, [O-methyl-11C]WAY-100635, in monkey and human plasma by HPLC: comparison of the behaviour of an identified radioactive metabolite with parent radioligand in monkey using PET. Nucl Med Biol.
10 Hall H, Lundkvist C, Halldin C, Farde L, Pike VW, McCarron JA, Fletcher A, Cliffe IA, Barf T, Wikstrom H, Sedvall G. (1997). Autoradiographic localization of 5-HT1A receptors in the post-mortem human brain using [3H]WAY-100635 and [11C]way-100635. Brain Res.
11 Pike V, McCarron JA, Hume SP, Asworth S, Opacka-Juffry J, Osman S, Lammertsma AA, Poole KG, Fletcher A, White AC, Cliffe IA. (1994). Preclinical development of a radioligand for studies of central 5-HT1a receptors in vivo - [11C]WAY-100635. Med Chem Res.
12 (1999).
13 McCarron J, Turton DR, Pike VWKG. (1996). Remotely controlled production of the 5-HT1A receptor radioligand, [carbonyl-11C]WAY100635, via 11C-carboxylation of an immobilized Grignard reagent J. Labelled Compd. Radiopharm.
Simpson NR, Montoya J, Mann JJ, Laruelle M. (1999). An improved one-pot procedure for the preparation of [11C-Carbonyl]-WAY100635. Nucl Med Biol.
15 Forster EA, Cliffe IA, Bill DJGM, Jones D, Reilly Y. (1995). Fletcher A A pharmacological profile of the selective silent 5-HT1A receptor antagonist, WAY-100635. Eur J Pharmacol.
16 Maeda J, Suhara T, Ogawa M, Okauchi T, Kawabe K, Zhang MR, Semba J, Suzuki K. (2001). In vivo binding properties of [carbonyl-11C]WAY-100635: effect of endogenous serotonin. Synapse.
17 Hume S, Hirani E, Opacka-Juffry J, Myers R, Townsend C, Pike V, Grasby P. (2001). Effect of 5-HT on binding of [(11)C] WAY 100635 to 5-HT(IA) receptors in rat brain, assessed using in vivo microdialysis nd PET after fenfluramine. Synapse.
18 Farde L, Ginovart N, Ito H, Lundkvist C, Pike VW, McCarron JA, Halldin C. (1997). PET-characterization of [carbonyl-11C]WAY-100635 binding to 5-HT1A receptors in the primate brain. Psychopharmacology (Berl).
19 Osman S, Lundkvist C, Pike VW, Halldin C, McCarron JA, Swahn CG, Farde L, Ginovart N, Luthra SK, Gunn RN, Bench CJ, Sargent PA, Grasby PM. (1998). Characterisation of the appearance of radioactive metabolites in monkey and human plasma from the 5-HT1A receptor radioligand, [carbonyl-11C]WAY-100635--explanation of high signal contrast in PET and an aid to biomathematical modelling. Nucl Med Biol.
20 Pike VW, McCarron JA, Lammerstma AA, Hume SPK, Grasby PM, Malizia A, Cliffe IA, Fletcher A, Bench CJ. (1995). First delineation of 5-HT1A receptors in human brain with PET and [11C]WAY-100635. Eur J Pharmacol.
21 Pike VW, McCarron JA, Lammertsma AA, Osman S, Hume SP, Sargent PA, Bench CJ, Cliffe IA, Fletcher A, Grasby PM. (1996). Exquisite delineation of 5-HT1A receptors in human brain with PET and [carbonyl-11 C]WAY-100635. Eur J Pharmacol.
22. Gunn RN, Sargent PA, Bench CJ, Rabiner EA, Osman S, Pike VW, Hume SP, Grasby PM, Lammertsma AA Tracer kinetic modeling of the 5-HT1A receptor ligand [carbonyl-11C]WAY-100635 for PET Neuroimage 1998;8(4):426–440.
23 Parsey RV, Slifstein M, Hwang DR, Abi-Dargham A, Simpson N, Mawlawi O, Guo NN, Van Heertum R, Mann JJ. (2000). Laruelle M Validation and reproducibility of measurement of 5-HT1A receptor parameters with [carbonyl-11C]WAY-100635 in humans: comparison of arterial and reference tisssue input functions. J Cereb Blood Flow Metab.
24 Parsey RV, Belanger MJ, Sullivan GM, Simpson NR, Sabin M, Heertum RV. (2005). Mann JJ Biodistribution and radiation dosimetry of 11C-WAY 100,635 in humans. J Nucl Med.
25 Sargent PA, Kjaer KH, Bench CJ, Rabiner EA, Messa C, Meyer J, Gunn RN, Grasby PM, Cowen PJ. (2000). Brain serotonin1A receptor binding measured by positron emission tomography with [11C]WAY-100635: effects of depression and antidepressant treatment. Arch Gen Psychiatry.
26 Bailer UF, Frank GK, Henry SE, Price JC, Meltzer CC, Weissfeld L, Mathis CA, Drevets WC, Wagner A, Hoge J, Ziolko SK, McConaha CW, Kaye WH. (2005). Altered brain serotonin 5-HT1A receptor binding after recovery from anorexia nervosa measured by positron emission tomography and [carbonyl11C]WAY-100635. Arch Gen Psychiatry.
27 Bhagwagar Z, Rabiner EA, Sargent PA, Grasby PM, Cowen PJ. (2004). Persistent reduction in brain serotonin1A receptor binding in recovered depressed men measured by positron emission tomography with [11C]WAY-100635. Mol Psychiatry.
28 Doder M, Rabiner EA, Turjanski N, Lees AJ, Brooks DJ. (2003). Tremor in Parkinson's disease and serotonergic dysfunction: an 11C-WAY 100635 PET study. Neurology.
29 Cleare AJ, Messa C, Rabiner EA. (2005). Grasby PM Brain 5-HT1A receptor binding in chronic fatigue syndrome measured using positron emission tomography and [11C]WAY-100635. Biol Psychiatry.
30 Savic I, Lindstrom P, Gulyas B, Halldin C, Andree B, Farde L. (2004). Limbic reductions of 5-HT1A receptor binding in human temporal lobe epilepsy. Neurology.
31 Meltzer CC, Price JC, Mathis CA, Butters MA, Ziolko SK, Moses-Kolko E, Mazumdar S, Mulsant BH, Houck PR, Lopresti BJ, Weissfeld LA. (2004). Reynolds CF Serotonin 1A receptor binding and treatment response in late-life depression. Neuropsychopharmacology.